# N,N´-Bis(2,3-dihydroxypropyl)-5-[N-(2-hydroxyethyl-3-methoxypropyl)-acetamidol]-2,4,6-triiodoisophthalamide

Chemical name: | N,N´-Bis(2,3-dihydroxypropyl)-5-[N-(2-hydroxyethyl-3-methoxypropyl)-acetamidol]-2,4,6-triiodoisophthalamide
Abbreviated name: | Iopentol
Synonym: | Imagopaque^®^, Ivepaque, Compound-5411, [underlined: 5-[Acetyl(2-hydroxy-3-methoxypropyl)amino]-][underlined: N][underlined: ,][underlined: N][underlined: '-bis(2,3-dihydroxypropyl)-2,4,6-triiodo-1,3-benzenedicarboxamide]
Agent Category: | Compound
Target: | Non-targeted agent, accumulation in the blood pool and extracellular space
Target Category: | Nonspecific filling of blood vessels and tissues
Method of detection: | X-ray, CT
Source of signal /contrast: | Iodine
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals; - Non-human primates; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%22iopentol%22%5BSubstance%20Name%5D%20OR%20Iopentol%5BText%20Word%5D%29%20OR%20%28%22iopentol%22%5BSubstance%20Name%5D%20OR%20Imagopaque%5BText%20Word%5D%29)]

N,N´-Bis(2,3-dihydroxypropyl)-5-[N-(2-hydroxyethyl-3-methoxypropyl)-acetamidol]-2,4,6-triiodoisophthalamide (iopentol) is a nonionic X-ray contrast agent used in various radiologic procedures to aid the radiographic visualization of selected tissues or organs.

X-Ray imaging (planar and tomographic) techniques depend on tissue density differences that provide the image contrast produced by X-ray attenuation between the area of interest and surrounding tissues (1, 2). Contrast enhancement (opacification) with use of contrast agents increases the degree of contrast and improves the differentiation of pathologic processes from normal tissues. Because iodine, an element of high atomic density, causes high attenuation of X-rays within the diagnostic energy spectrum, water-soluble and reasonably safe iodinated contrast agents in intravenous injectable forms have been developed for clinical applications (3, 4).

Water-soluble, intravenous X-ray contrast agents are generally organic iodine compounds that contain one or more tri-iodinated benzene rings (5, 6). When injected intravenously, they are largely distributed in the extracellular fluid space and excreted unchanged by the kidneys (7). Contrast enhancement of a region of interest depends on the route of administration, delivery of the agent to the area by blood flow, and the final iodine concentration in the region. There are two basic types of these compounds: ionic and nonionic agents. The first monomeric ionic compound, in the form of 2,4,6-triiodobenzene acetrizoic acid, was synthesized by Wallingford (3). Most ionic contrast agents are derived from the basic structures of 3,5-diamino-2,4,6-triiodobenzoic acid, 5-amino-2,4,5-triiodoisophthalic acid, or 2,4,6-triiodobenzene-1,3,5-tricarbonic acid. In addition to monoacidic ionic dimers, nonionic compounds have also been developed to improve the tolerability of these agents in patients. The basic strategy of developing nonionic agents is to eliminate the electrical charges in the structure, which will lead to a reduction in osmolality of the compound. Because osmolality is related to the number of particles in solution, the challenge is to reduce the number of particles but maintain the iodine concentration (8). This was generally achieved by conversion of the carboxyl groups to hydroxyalkylamide groups (9). Further improvement was made by replacing the amino sugar with aminoalcohols to produce heat-stable hydroxyalkylamides to allow product sterilization (10).

As a low-osmolar nonionic monomer, iopentol was developed in an effort to increase the safety and tolerance of X-ray contrast agents. Chemically, it is a m-carboxamido-O-iodo-N-(β-hydroxyalkyl)aniline derivative and a water-soluble ratio 3.0 (3 iodine atoms to 1 osmotic particle) compound (11, 12). Iopentol is not commercially available in the United States. It has been used in Europe for arteriography, urography, phlebography and computed tomography enhancement, arthrography, endoscopic retrograde cholangiopancreatography, hysterosalpingography, and gastrointestinal studies. The commercial preparations were available in iodine concentrations ranging from 150 to 350 mg/ml (13).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28Iopentol%20OR%20imagopaque%29%20AND%20synthesis)]

The synthesis steps involved in the production of X-ray contrast agents are well-established organic reactions (5). Hoey et al. (14) described the basic approach of synthesizing derivatives of isophthalamic acid as contrast agents. Berg and Fagervoll (15) and Haavaldsen et al. (16) reported the synthesis of iopentol by treating dimethyl 5-nitroisophthalate with 3-amino-1,2-propanediol in boiling methanol and refluxing for 24 h to produce the corresponding isophthalamide. This product was hydrogenated in the presence of 10% palladium/charcoal in a Parr apparatus for 1 day at room temperature to give the aminoisophthalamide. Iodination followed by acetylation gave the acetamido derivative, which was alkylated with 1-chloro-3-methoxy-2-propanol in a suitable solvent, such as methanol or propylene glycol, under basic conditions. This final step yielded ~70% iopentol. Because of the use of racemic mixtures of chiral reagents during synthesis, the final product consisted of several diastereomers. In another report, Berg et al. (17) identified, synthesized, and characterized several potential impurities for quality control purposes.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28Iopentol%20OR%20imagopaque%29%20AND%20%28%22in%20vitro%22%29)]

Skinnemoen (18) studied the in vitro physicochemical properties of iopentol and determined that the osmolality and viscosity of iopentol ranged from 0.31 osmoles/kg H_2_O and 2.7 mPa·s at 37 ºC for the150 mg iodine/ml concentration to 0.81 osmoles/kg H_2_O and 26.6 mPa·s at 37 °C for the 350 mg iodine/ml concentration. In comparison, for iohexol (a nonionic contrast agent) at a concentration of 350 mg iodine/ml, the values were 0.78 osmoles/kg H_2_O and 23.3 mPa·s. The 1-octanol:water partition coefficients for iopentol and iohexol were 0.007 and 0.001, respectively.

Krause et al. (19) investigated the biochemical properties of 11 ionic and nonionic contrast agents. The lowest protein binding values were obtained for iopentol and iomeprol. In a histamine release study using rat mast cells, iopentol and other nonionic contrast agents released less than 12% of histamine at the 100 mg iodine/ml concentration. At the same concentration, diatrizoate, an ionic contrast agent, released 77.5% of histamine. Iopentol and iotetrol showed the highest influence on complement activation (77 and 71% inhibition, respectively, at 100 mg iodine/ml). The lowest effect was observed for iopamidol (0%) and diatrizoate.

In a series of in vitro studies (20-22), the effects of iopentol and other nonionic contrast agents (iohexol, iodixanol, and iopamidol) on red blood cells were investigated. A microscopy study revealed that all contrast agents induced morphologic changes with small differences among the agents. The changes appeared to be related to the osmolality of the tested solution. The authors of the study suggested that the changes were most likely of small clinical importance. All contrast agents decreased red blood cell aggregation with no differences among the various agents. The authors suggested that the chemotoxic effect had more impact than the osmolality on red blood cell aggregation. No difference was found among the agents in the effect on red blood cell rigidification. Diatrizoate did induce significantly more red blood cell rigidity when compared with the nonionic agents.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28Iopentol%20OR%20imagopaque%29%20AND%20rodentia)]

Michelet and Skinnemoen (23) examined the pharmacokinetics of iopentol in rats by injecting [^125^I]iopentol (specific activity = 2 kBq (0.05 μCi)/kg) at a dose of 200 mg iodine/kg into the caudal vein. After injection, the blood radioactivity level decreased rapidly with time and approached zero after 1-2 h. The blood elimination half-life (t_½_) was 24.4 ± 6.3 min (n = 5). About 86.8 ± 3.8% (n = 10) of the injected dose (ID) and 12.7 ± 2.0% ID were found in urine and feces at 24 h, respectively. Most organs did not contain any detectable activity. The concentration in the thyroid was 31.6 ± 10.0 iodine/g wet tissue. The highest tissue concentrations were 89.2 ± 40.8 and 314.3 ± 163.7 μg iodine/g wet tissue in the gastrointestinal tract at 24 h and 7 days, respectively. High-performance liquid chromatography (HPLC) analysis of the urine (pooled samples from 0 to 48 h) did not detect any possible metabolites from deiodination. At a higher dose of 10 g iodine/kg, the level of deiodination products was estimated to be 0.1% ID. HPLC analysis of the bile (pooled samples from 0 to 180 min) showed that a minimum of 4.6% ID was excreted unchanged.

In a study of acute toxicity at the 350 mg iodine/ml concentration of iopentol, Michelet et al. (24) reported an acute i.v. median lethal dose (LD_50_) of 19.5 g iodine/kg for doses between 17.5 and 24.5 g iodine/kg in male mice and an LD_50_ of 119.4 g iodine/kg for doses between 17.5 and 24.5 g iodine/kg in female mice. The acute i.v. LD_50_ of iopentol in rats was 10.3-11.7 g iodine/kg for doses between 8.75 and 15.75 g iodine/kg. For the same concentration and doses, the LD_50_s were 11.7-12.1 and 10.3-10.8 g iodine/kg for iohexol and iopamidol, respectively. Heywood et al. (25) reported a summary of the toxicologic profile of iopentol and found that the only significant finding in the repeat-dose studies in rats was cytoplasmic vacuolation in the kidney proximal tubules at the highest dose level (4 g iodine/kg/day) for 4 weeks. This effect was reversible within 14 days. The battery of mutagenic tests showed no genotoxic or clastogenic potential for iopentol. No teratogenic effects and other adverse effects of importance were observed on any of the measured characteristics of reproduction.

Luzzani et al. (26) reported the LD_50_ values of intracisternal injection in rats and intracerebroventricular injection in mice for nonionic monomers (iomeprol, iopamidol, iohexol, iopentol, and iopromide) and dimers (iofratol, iotrolan, and iodixanol). For iopentol, the intracerebroventricular LD_50_ in mice was 1.11-1.24 g iodine/kg, and the intracisternal LD_50_ in rats was 0.15-0.34 g iodine/kg. In comparison, iohexol had values of 0.69-1.00 and >1.50 g iodine/kg, respectively. Iodixanol had values of 0.88-1.06 and >1.60 g iodine/kg, respectively.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28iopentol%20OR%20imagopqaue%29%20AND%20%28dog%20OR%20pig%20OR%20rabbit%20OR%20sheep%29)]

Leunbach et al. (27) studied the metabolism and excretion of iopentol (350 mg iodine/ml concentration and 1 g iodine/kg dose) in pigs. The iodine concentration in the urine increased from 46-113 mg iodine/ml at 0-2 h to 64-118 mg iodine/ml at 2-4 h and then decreased to 2-33 mg iodine/ml at 10-12 h. The iodine concentration in bile increased from 2.4-3.0 to 2.2-3.4 mg iodine/ml and then decreased to 0.1-0.7 mg iodine/ml at 10-12 h. Most of the compound appeared to be excreted in urine during the first 12 h. The amounts of metabolites in the 24 h urine and bile samples were 0.2-0.8 and 0.02-4.7 mg iodine/ml, respectively.

Michelet (28) studied the effect of intravascular contrast media on the rabbit blood-brain barrier (BBB) after intracarotid injection of iopentol, iohexol, iothalamate, and iodixanol. BBB injuries were demonstrated by the extravasation of ^99m^Tc-pentetate (^99m^Tc-DTPA; reversible changes), ^125^I-labeled human serum albumin (^125^I-HSA; severe permeability disturbances), and Trypsin blue. The results were expressed as percentage of increased radioactivity in the injected hemisphere over the amount in the non-injected hemisphere. All contrast agents had increased mean values of ^99m^Tc-DTPA extravasation in the injected hemisphere compared with the contralateral hemisphere. For iopentol, the extravasation of ^99m^Tc-DTPA and ^125^I-HSA was 137 ± 75 and 9 ± 16%, respectively. In comparison, the values for iohexol were 128 ± 39 and 32 ± 15%, respectively. The values for iothalamate (ionic monomer) were 475 ± 118 and 215 ± 68%, respectively.

Sunnegardh et al. (29) reported that both iopentol and iohexol (at 300 mg iodine/ml concentration and 4 ml/kg dose) had similar pulmonary and renal hemodynamic effects in pigs. Renal venous blood flow and vascular resistance were not significantly changed. Both induced a significant increase in pulmonary arterial occlusion pressure and cardiac output.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28Iopentol%20OR%20imagopaque%29%20AND%20%28primate%20NOT%20human%29)]

Heywood et al. (25) performed a toxicity study of iopentol at dosage levels of 0.5, 1.5, and 3.0 g iodine/kg in 24 cynomolgus monkeys for 28 days. There were no deaths and no overt signs of toxicity. Hematology, biochemistry, and urinalysis did not show any significant differences of toxicologic importance. Cytoplasmic vacuolations were found in kidney proximal tubules. Coarse vacuolation of centrilobular hepatocytes and islet cells were observed in animals that received the highest dose (3 g iodine/kg).

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28Iopentol%20OR%20imagopaque%29%20AND%20humans)]

Waaler et al. (30) conducted a pharmacokinetic study of 3 dose levels of iopentol in 24 healthy volunteers. Iopentol was given in the concentration of 350 mg iodine/ml. No significant dose effect was observed on the iopentol pharmacokinetics. The serum concentration of iopentol decreased biexponentially. The volume of distribution corresponded approximately to that of the extracellular fluid. Unmetabolized iopentol was excreted almost entirely in urine during the first 24 h. The authors observed that this was different from rat studies in that a high fraction of iopentol was excreted in the feces by rats. The overall mean values (95% confidence interval; n =24) of the initial distribution half-life (t_½α_), elimination half-life (t_½β_), the apparent volumes of distribution, and renal clearances were 23 (21.1-25.5) min, 121 (115.9-125.8) min, 18.4 (17.3-19.5) liters, and 104 (97-111) ml/min, respectively. After 24 h, 98% of the dose was accumulated in the urine and no metabolites were detected. On the basis of ^51^Cr-EDTA studies, the authors indicated that the mechanism of iopentol excretion was glomerular filtration.

The pharmacologic effects of iopentol were studied by Aakhus et al. (31) in 24 healthy volunteers. Iopentol was well tolerated when injected i.v. in doses of 300 to 1,200 mg iodine/kg. No changes were observed in blood pressure and electrocardiograms with a clinically insignificant increase in heart rate. Five subjects reported headache, and a mild sensation of warmth was reported by 13 subjects. The majority of the clinical-chemical observations did not show any statistically significant changes. A slight increase was demonstrated in the serum thyrotropin level. In phase I and II clinical trials, Jakobsen et al. (32) and Andrew et al. (12) reported no severe or unexpected adverse events. Jakobsen et al. (33) studied the renal effects of iopentol and iohexol (350 mg iodine/ml concentration and dose of 700 mg iodine/kg) in 64 patients and found no significant difference between iopentol and iohexol. Both agents had no significant effects on creatinine clearance and the mean serum values of creatinine, urea, and β_2_-microglobulin.

In a randomized, double-blind, parallel phase III clinical trial, 149 patients received iopentol (300 mg iodine/ml) and 150 patients received iohexol (300 mg iodine/ml) for urography, Rasmussen et al. (34) reported that there was no significant difference between the two agents. There appeared to be a trend for iopentol to increase the heart rate and iohexol to decrease the heart rate, but no significant difference in the heart rate was observed between the two groups. No change in blood pressure was observed in both groups. Seven patients (5%) in the iohexol group and 12 patients (8%) in the iopentol group experienced mild adverse effects other than a sensation of warmth. Only 1 patient in the iopentol group complained of a severe headache. In the diagnostic efficacy study, 86% of the iopentol group and 81% of the iohexol group received an excellent grade in the overall quality of visualization. Only 3% and 2% received a poor grade for the iopentol and iohexol group, respectively.

Various other studies [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28Iopentol%29%20AND%20%28iohexol%20OR%20ioxaglate%20OR%20amidotrizoate%20OR%20iopromide%20OR%20iodixanol%20OR%20metrizoate%29)] have indicated that iopentol has safety and efficacy profiles similar those for other nonionic contrast agents.

## References

1. Swanson, D.P. and M.B. Alpern, Contrast media for computed tomography: Intravascular, intracavitary, xenon, reticuloendothelial, in Pharmaceuticals in medical imaging, D.P. Swanson, H. M. Chilton and J. H. Thrall, Editor. 1990, Macmillan Publishing Company: New York. p. 99-124.
2. Hoey, G.B. and K.R. Smith, Chemistry of X-ray contras media, in Radiocontrast agents, M. Sovak, Editor. 1984, Springer-Verlag: New York. p. 23-125.
3 Wallingford V.H. (1953). The development of organic iodine compounds as x-ray contrast media. J Am Pharm Assoc Am Pharm Assoc (Baltim).
4 Sovak M., Ranganathan R., Lang J.H., Lasser E.C. (1977). and Concepts in design of improved intravascular contrast agents. European Society of cardiovascular Radiology, Uppsala, (May): p. 25-27.
5. Gries, H., Chemistry of X-ray contrast agents, in Textbook of contrast media, P. Dawson, D.O. Cosgrove, and R.G. Grainger, Editors. 1999, Isis Medical Media Ltd.: Oxford. p. 15-22.
6 Almen T. (1969). Contrast agent design. Some aspects on the synthesis of water soluble contrast agents of low osmolality. J Theor Biol.
7. Dawson, P., Pharmacokinetics of water-soluble iodinated X-ray contrast agents, in Textbook of contrast media, P. Dawson, D.O. Cosgrove, and R.G. Grainger, Editors. 1999, Isis Medical Media Oxford. p. 61-74.
8 Ralston W.H., Robbins M.S., Coveney J., Blair M. (1989). Acute and subacute toxicity studies of ioversol in experimental animals. Invest Radiol.
9 Almen T. Development of nonionic contrast media Invest Radiol 1985 20Suppl1 S2 9 2579043
10 Sovak M. Ranganathan R. Stability of nonionic water-soluble contrast media: implications for their design Invest Radiol 1980 15Suppl6 S323 8 7203944
11 Almen T., Baath L. (1987). Effects of iopentol, iohexol and metrizoate on the contractility of the isolated rabbit heart. Acta Radiol Suppl.
12 Andrew E., Waaler A., Jakobsen J., Holager T., Lambrechts M., Moxnes A., Kruger Hagen E., Bach-Gansmo T. (1988). Clinical trial program for iopentol. A new nonionic ratio 3.0 contrast medium with emphasis on clinical phases I and II. Invest Radiol.
13 (2004). Imagopaque 250 mg I/ml solution for injection, Irish Medicines Board. p. 1-8.
14. Hoey, G.B., R.D. Rands, G. DeLaMater, D.W. Chapman, and P.E. Wiegert, Synthesis of derivatives of isophthalamic acid as X-ray contrast agents. 1963.
15 Berg A., Fagervoll R. (1987). Synthesis, isomerism and characterization of iopentol. Acta Radiol Suppl.
16 Haavaldsen J., Nordal V., Kelly M. (1983). X-ray contrast agents. I. Synthesis of some derivatives of 5-amino-2,4,6-triiodoisophthalamide. Acta Pharm Suec.
17 Berg A., Fagervoll R., Aulie Michelet A., Dugstad H. (1987). Synthesis, analysis and toxicity of some compounds which may be formed during the synthesis of iopentol. Acta Radiol Suppl.
18 Skinnemoen K. (1987). Physicochemical properties and degree of protein binding of iopentol. Acta Radiol Suppl.
19 Krause W., Miklautz H., Kollenkirchen U., Heimann G. (1994). Physicochemical parameters of x-ray contrast media. Invest Radiol.
20 Aspelin P., Nilsson P.E., Schmid-Schonbein H., Schroder S., Simon R. (1987). Effect of four non-ionic contrast media on red blood cells in vitro. III. Deformability. Acta Radiol Suppl.
21 Aspelin P., Nilsson P.E., Schmid-Schonbein H., Schroder S., Simon R. (1987). Effect of four non-ionic contrast media on red blood cells in vitro. I. Morphology. Acta Radiol Suppl.
22 Aspelin P., Nilsson P.E., Schmid-Schonbein H., Schroder S., Simon R. (1987). Effect of four non-ionic contrast media on red blood cells in vitro. II. Aggregation. Acta Radiol Suppl.
23 Michelet A.A., Skinnemoen K. (1987). Pharmacokinetics of iopentol in the rat. Acta Radiol Suppl.
24 Michelet A.A., Salvesen S., Renaa T. (1987). Acute toxicity of iopentol in rodents. Acta Radiol Suppl.
25 Heywood R., Mayfield R., Allan J.A., Michelet A.A. (1987). Summary of the toxicologic profile of iopentol. Acta Radiol Suppl.
26 Luzzani F., Morisetti A., Bussi S., Tirone P., de Haen C. (1996). Neurotolerability of nonionic X-ray contrast media. The role of chemotoxicity. Invest Radiol.
27 Leunbach I., Skinnemoen K., Golman K. (1987). Metabolism and excretion of iopentol in the pig. Acta Radiol Suppl.
28 Michelet A.A. (1987). Effects of intravascular contrast media on blood-brain barrier. Acta Radiologica.
29 Sunnegardh O., Hietala S.O., Wirell S., Ekelund L. (1990). Systemic, pulmonary and renal haemodynamic effects of intravenously infused iopentol. A comparison in the pig of a new low osmolar non-ionic medium with saline and iohexol. Acta Radiol.
30 Waaler A., Jorgensen N.P., Koksvik B., Skinnemoen K., Andrew E. (1987). Pharmacokinetics of iopentol in healthy volunteers. Acta Radiol Suppl.
31 Aakhus T., Stokke O., Stormorken H., Berg K.J., Dahlstrom K. (1987). Pharmacologic effects of iopentol after intravenous injection in healthy volunteers. Preliminary report. Acta Radiol Suppl.
32 Jakobsen J.A., Hagve T.A., Holager T., Waaler A., Haider T., Andrew E., Aakhus T. (1989). Safety and toleration of the non-ionic contrast medium iopentol. An intravenous phase I trial. Eur J Radiol.
33 Jakobsen J.A., Kolbenstvedt A.N., Berg K.J. (1991). Renal effects of iopentol and iohexol after intravenous injection. Acta Radiol.
34 Rasmussen F., Dyreborg U., Larsen C., Waaler A., Tove Kristofferson D. (1990). Intravenous urography with a new non-ionic contrast media in a clinical phase III study: iopentol vs iohexol. Clin Radiol.